# 1-(3-[^11^C]Methoxy-4-methoxybenzyl)-6,7-dimethoxyisoquinoline

Chemical name: | 1-(3-[^11^C]Methoxy-4-methoxybenzyl)-6,7-dimethoxyisoquinoline
Abbreviated name: | [^11^C]Papaverine
Synonym:
Agent category: | Compound
Target: | Phosphodiesterase type 10A
Target category: | Enzyme binding
Method of detection: | Positron emission tomography, PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Carbon-11%20Papaverine)]

Phosphodiesterases (PDEs) are composed of at least 11 families of enzymes that hydrolyze cyclic 3´,5´-adenosine monophosphate (cAMP) and/or cyclic 3´,5´-guanosine monophosphate (cGMP) to the corresponding inactive 5´-AMP and 5´-GMP, respectively (1, 2). These second-messenger cyclic nucleotides are formed in response to stimuli (such as hormones, neurotransmitters, and cytokines) to regulate cellular functions. PDEs are essential in the termination of cellular responses via their degradation of cyclic nucleotides. PDE type-10A (PDE10A) is a dual-specificity PDE that can act on both cAMP and cGMP (3). PDE10A is found mainly in the brain (striatum) and testes, with low concentrations in other tissues (4). PDE10A may play a role in the regulation of glutamatergic and dopaminergic functions in neurons (5, 6). PDE10A inhibitors have been studied in the new treatment of neuropsychiatric disorders such as schizophrenia, Huntington’s disease, Parkinson’s disease, obsessive-compulsive disorder, and addiction (7-11).

1-(3,4-Dimethoxybenzyl)-6,7-dimethoxyisoquinoline (papaverine) has been found to be a specific inhibitor of PDE10A (9). 1-(3-[^11^C]Methoxy-4-methoxybenzyl)-6,7-dimethoxyisoquinoline ([^11^C]Papaverine) has been evaluated as a positron emission tomography (12) agent for the non-invasive study of PDE10A in the brain in rats and monkeys (13). However, the results of these studies indicated that the rapid brain washout of the tracer limits its utility as a PET agent for in vivo measurements of PDE10A.

### Related Resource Links:

- Chapters in MICAD (PDE (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=PDE+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (PDE10A (http://www.ncbi.nlm.nih.gov/gene/10846))
- Articles in Online Mendelian Inheritance in Man (OMIM) (PDE10A (http://www.ncbi.nlm.nih.gov/omim/610652))
- Clinical trials (Papaverine (http://www.clinicaltrials.gov/ct2/results?term=Papaverine))
- Drug information in FDA (Papaverine (http://google2.fda.gov/search?q=papaverine&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=13))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Carbon-11%20Papaverine%20and%20synthesis)]

Tu et al. (13) synthesized [^11^C]papaverine by O-methylation of the desmethyl precursor 4-((6,7-dimethoxyisoquinolin-1-yl)methyl)-2-methoxyphenol with [^11^C]methyl iodide at 85°C for 5 min. Subsequent separation with high-performance liquid chromatography produced a radiochemical purity >99%. The decay-corrected specific activity was 740 GBq/μmol (20 Ci/µmol; n = 5) at the end of bombardment with a radiochemical yield of 70% based on [^11^C]methyl iodide. Total synthesis time was 50–55 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Carbon-11%20Papaverine%20and%20in%20vitro)]

Siuciak et al. (9) showed that papaverine was a specific inhibitor of PDE10A with IC_50_ values of 36 nM, 1,300 nM, and 320 nM for PDE10A, PDE3A, and PDE4D, respectively. Tu et al. (13) used autoradiography to show that [^11^C]papaverine binding occurred mainly in the striatum of the rat brain and in the caudate and putamen of rhesus macaque brain sections.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Carbon-11%20Papaverine%20and%20rodentia)]

Ex vivo biodistribution studies in normal rats showed high accumulation of radioactivity in the liver at 5 min after injection of [^11^C]papaverine, followed by the kidney and brain (13). [^11^C]Papaverine accumulation at 5 min after injection was highest in the striatum (0.200% injected dose (ID)/g) and lower in the hippocampus (0.188% ID/g), cerebellum (0.161% ID/g), and cortex (0.144% ID/g), as predicted by the density of PDE10A enzymes. However, radioactivity distribution became homogenous due to rapid washout in all brain regions at 30 min after injection. There was ~22% intact [^11^C]papaverine in the plasma at 30 min after injection, with one major radioactive hydrophilic metabolite. In the brain, 96% of [^11^C]papaverine was intact at 7 min after injection. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Carbon-11%20Papaverine%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Carbon-11%20Papaverine%20and%20%28primate%20not%20human%29)]

Tu et al. (13) obtained serial brain PET scans in two male rhesus macaque monkeys after injection of 370 MBq (10 mCi) [^11^C]papaverine. Accumulation in the brain rapidly peaked at 3 min after injection, with standard uptake values of 3.2 in the putamen, 2.5 in the caudate, and 2.2 in the cerebellum. No significant accumulation was observed in the other brain regions. There were rapid decreases in radioactivity in all brain regions by 10 min after injection. The putamen/cerebellum and caudate/cerebellum ratios were ~1 at 10 min after injection. The investigators concluded that [^11^C]papaverine is not a useful PET radioligand for PED10A imaging in the brain.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Carbon-11%20Papaverine%20and%20human)]

No publication is currently available.

## NIH Support

DA16181, NS48056

## References

1 Sutherland E.W., Rall T.W. (1958). Fractionation and characterization of a cyclic adenine ribonucleotide formed by tissue particles. J Biol Chem.
2 Essayan D.M. (2001). Cyclic nucleotide phosphodiesterases. J Allergy Clin Immunol.
3 Fujishige K., Kotera J., Michibata H., Yuasa K., Takebayashi S., Okumura K., Omori K. (1999). Cloning and characterization of a novel human phosphodiesterase that hydrolyzes both cAMP and cGMP (PDE10A). J Biol Chem.
4 Fujishige K., Kotera J., Omori K. (1999). Striatum- and testis-specific phosphodiesterase PDE10A isolation and characterization of a rat PDE10A. Eur J Biochem.
5 Nishi A., Kuroiwa M., Shuto T. (2010). Role of phosphodiesterases in dopamine signal transduction. Nippon Yakurigaku Zasshi.
6 Xie Z., Adamowicz W.O., Eldred W.D., Jakowski A.B., Kleiman R.J., Morton D.G., Stephenson D.T., Strick C.A., Williams R.D., Menniti F.S. (2006). Cellular and subcellular localization of PDE10A, a striatum-enriched phosphodiesterase. Neuroscience.
7 Kehler J., Kilburn J.P. (2009). Patented PDE10A inhibitors: novel compounds since 2007. Expert Opin Ther Pat.
8 Chappie T., Humphrey J., Menniti F., Schmidt C. (2009). PDE10A inhibitors: an assessment of the current CNS drug discovery landscape. Curr Opin Drug Discov Devel.
9 Siuciak J.A. (2008). The role of phosphodiesterases in schizophrenia : therapeutic implications. CNS Drugs.
10 Menniti F.S., Chappie T.A., Humphrey J.M., Schmidt C.J. (2007). Phosphodiesterase 10A inhibitors: a novel approach to the treatment of the symptoms of schizophrenia. Curr Opin Investig Drugs.
11 Hebb A.L., Robertson H.A. (2007). Role of phosphodiesterases in neurological and psychiatric disease. Curr Opin Pharmacol.
12 Gao X., Yang L., Petros J.A., Marshall F.F., Simons J.W., Nie S. (2005). In vivo molecular and cellular imaging with quantum dots. Curr Opin Biotechnol.
13 Tu Z., Xu J., Jones L.A., Li S., Mach R.H. (2010). Carbon-11 labeled papaverine as a PET tracer for imaging PDE10A: radiosynthesis, in vitro and in vivo evaluation. Nucl Med Biol.